# [^18^F]1-(2-Fluoroethyl)-4-[(4-cyanophenoxy)methyl]piperidine

Chemical name: | [^18^F]1-(2-Fluoroethyl)-4-[(4-cyanophenoxy)methyl]piperidine
Abbreviated name: | [^18^F]SFE
Synonym: | [^18^F]WLS1.002, [^18^F]-2
Agent Category: | Compound
Target: | Sigma (σ) receptor
Target Category: | Receptor binding
Method of detection: | Positron Emission Tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%5DSFE%20OR%20%5B18F%5D-2%20OR%20%5B18F%5DWLS1.002%20OR%20%28sigma%201%20receptor%20radioligand%29)]

[^18^F]1-(2-Fluoroethyl)-4-[4-cyanophenoxy)methyl]piperidine ([^18^F]SFE) is a radioligand developed for positron emission tomography (PET) imaging of the sigma (σ) receptors (1-3). ^18^F]SFE is a potent σ_1_ receptor agonist labeled with ^18^F, a positron emitter with a physical half-life (t_½_) of 109.8 min.

σ receptors are functional, membrane-bound, G-protein-coupled receptors distributed in the central nervous system (CNS) and peripheral organs (4). The CNS σ receptors are unique binding sites related to higher brain functions (5). They are distinct from opiate and phencyclidine binding sites. There are at least two subtypes of sigma receptors, σ_1_ and σ_2_ receptors. The precise mechanism of the functional response of these receptors is not entirely known. These receptors appear to be involved in numerous pharmacological and physiological functions, and they also modulate a number of central neurotransmitter systems, including noradrenergic, glutamatergic, and dopaminergic systems. Phencyclidine and derivatives, cocaine and derivatives, some neuroleptics, atypical antipsychotic agents, and other chemically unrelated compounds can bind to the σ receptor sites. Studies have shown that these receptors may play a role in the pathogenesis of psychiatric disorders (6, 7). These receptors are also expressed on a number of human and murine tumors (8).

The σ_1_ receptor subtypes have a molecular weight of ≈25 kDa, and through the process of cloning they have shown a 30% sequence homology with the yeast C89-C7 sterol isomerase (4, 9, 10). The σ_2_ receptor subtypes have a molecular weight of ≈21.5 kDa, and have not been cloned. The σ_1_ receptors are thought to be involved in certain neuropsychiatric disorders, and the σ_2_ receptors are also implicated in malignant neoplastic diseases. Because of these effects, σ receptor ligands may be useful for detection and treatment in neurology and oncology. A number of ligands for these receptors have been labeled with ^11^C and ^18^F for PET imaging to map their in vivo brain distribution and expression on tumors (11). Waterhouse et al. (12, 13) synthesized a number of selective σ_1_ receptor ligands for both PET and single-photon emission computed tomography. [^18^F]1-(3-Fluoropropyl)-4-(4-cyanophenoxy-methyl)piperidine ([^18^F]FPS) was found to be a high-affinity σ_1_ receptor ligand with a dissociation constant (K_d_) of 0.5 nM, but it was not cleared fast enough from the CNS to reach transient equilibrium by 4 h after administration in healthy volunteers (3). In an effort to improve the CNS clearance for in vivo PET studies, Zhao et al. (3) synthesized and evaluated [^18^F]SFE (K_d_ = 5 nM), a analog of [^18^F]FPS analog that exhibits a lower affinity for σ_1_ receptor ligands.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B18F%5DSFE%20OR%20%5B18F%5D-2%20OR%20%5B18F%5DWLS1.002%20OR%20%28sigma%201%20receptor%20radioligand%29%29%20AND%20synthesis)]

Zhao et al. (3) reported the synthesis of [^18^F]SFE from 4-(4-cyanophenoxy)methyl)piperidine, which was first prepared from ethyl isonepecotate in a five-step method. Alkylation of 4-(4-cyanophenoxy)methyl)piperidine with 2-bromo-1-ethanol in potassium carbonate and dichloromethane resulted in a 72%yield of the intermediate compound, 1-(2-hydroxyethyl)-4-[(4-cyanophenoxy)methyl]piperidine. The alkyl mesylate precursor for [^18^F]SFE was obtained by treating this intermediate compound with methanesulfonyl chloride in triethylamine and dichloromethane (64% yield). Radiosynthesis of [^18^F]SFE was carried out by heating the alkyl mesylate precursor at 90ºC for 15 min in an anhydrous solution of [^18^F]fluoride and Kryptofix-potassium carbonate mixture in acetonitrile. Deionized water was added, and the mixture was heated for another 10 min to convert the unreacted precursor to the corresponding alcohol for easy purification. [^18^F]SFE was obtained after purification by high-performance liquid chromatography (HPLC) with a yield of 59 ± 8% (n = 6) at the end of bombardment. The average time of synthesis was ≈100 min. The radiochemical purity was 98.3 ± 2.1%, and the specific activity was 106.93 ± 23.68 GBq/μmol (2.89 ± 0.80 Ci/μmol) at the end of synthesis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B18F%5DSFE%20OR%20%5B18F%5D-2%20OR%20%5B18F%5DWLS1.002%20OR%20%28sigma%201%20receptor%20radioligand%29%29%20AND%20in%20vitro)]

Waterhouse et al. (12) reported in vitro receptor binding assays for several σ ligands in guinea pig membranes. The inhibition constant (K_i_) of SFE for σ_1_ receptors was 24.3 nM, and the K_i_ for σ_2_ receptors was 361 nM. The K_i_ values of FPS were 4.3 and 144 nM for σ_1_ and σ_2_ receptors, respectively. Zhao et al. (3) conducted in vitro competitive binding assays of SFE in rat forebrain membranes. K_d_ for SFE was 5.0 nM, in comparison, the K_d_ for FPS was 0.5 nM. The lipophilicity (log P) of SFE was estimated to be 2.42 based on its retention time in a C18 column as compared to standards of known log P values.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B18F%5DSFE%20OR%20%5B18F%5D-2%20OR%20%5B18F%5DWLS1.002%20OR%20%28sigma%201%20receptor%20radioligand%29%29%20AND%20rodentia)]

Zhao et al. (3) injected 555 kBq (15 μCi) [^18^F]SFE into awake male rats (n = 4-5) for biodistribution and blocking studies. The whole-brain radioactivity concentrations, measured as percentage of injected dose per g (% ID/g) were 1.41 ± 0.05% ID/g, 1.08 ± 0.23% ID/g, and 0.33 ± 0.053% ID/g at 5 min, 60 min, and 330 min, respectively. At 5 min, the radioactivity concentrations (% ID/g) in major organs were 7.71 ± 0.93 (lung), 2.99 ± 0.10 (kidney), 1.75 ± 0.15 (heart), 1.40 ± 0.32 (intestine), 1.01 ± 0.21(spleen), 0.68 ± 0.17 (liver), and 0.14 ± 0.03% (blood). Except for the liver, radioactivity was cleared rapidly. The rapid biological clearance t_½_ phase was 0.1−0.2 h, and the slow biological clearance t_½_ phase was 2−4 h. The relative radioactivity concentration in the bone was low and did not significantly increase over time. Administration of the a σ_1_ receptor selective compound (BD1008) 5 min before [^18^F]SFE administration reduced brain activity by 80% at 60 min.

Waterhouse et al. (1) reported regional brain radioactivity concentrations in four rats. Each rat received 555−740 kBq (15−20 μCi) [^18^F]SFE. The specific activity was 88.8 ± 22.2 GBq/μmol (2.4 ± 0.6 Ci/μmol) at the end of synthesis. The rats were euthanized and specific brain regions were dissected and assayed. The regional brain radioactivity concentrations (% ID/g; n = 4) at 5 min were 2.02 ± 0.41 (occipital cortex), 2.00 ± 0.38 (frontal cortex), 1.66 ± 0.76 (striatum), 1.25 ± 0.25 (thalamus), 1.18 ± 0.19 (cerebellum), and 0.99 ± 0.19 (hippocampus). This appeared to be consistent with previously reported CNS σ_1_ receptor distribution pattern. At 60 min, these values decreased (% ID/g) to 1.28 ± 0.08 (occipital cortex), 1.42 ± 0.12 (frontal cortex), 1.01 ± 0.06 (striatum), 1.14 ± 0.10 (thalamus), 0.96 ± 0.03 (cerebellum), and 0.87 ± 0.08 (hippocampus). Pretreatment with unlabeled SFE, FPS, and BD1407 (σ_1-_selective) reduced regional brain radioactivity by ≈80%. The brain metabolite study by HPLC analysis (n = 3) at 60 min showed that the percentages of unchanged [^18^F]SFE were 53 ± 5, 93 ± 1, and 97 ± 1 in the plasma, frontal cortex, and cerebellum, respectively.

Based on the rat [^18^F]SFE distribution data from rats, Waterhouse et al. (2) reported human dosimetry estimation extrapolated from organs and the whole body. Organs with significant radioactivity generally received ≈0.02−0.04 mGy/MBq (0.054−0.108 rad/mCi). The adrenal gland was the critical organ with the highest dose of 0.044 mGy/MBq (0.163 rad/mCi), The doses of other major organs in mGy/MBq (rad/mCi) were 0.0238 (0.88), 0.0397 (0.147), 0.0382 (0.141), 0.03 (0.111), and 0.0284 (0.105) for the brain, lungs, liver, spleen, and kidneys, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B18F%5DSFE%20OR%20%5B18F%5D-2%20OR%20%5B18F%5DWLS1.002%20OR%20%28sigma%201%20receptor%20radioligand%29%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

Waterhouse et al. (2) studied the potential toxic effects of SFE in rabbits. The rabbits received i.v. doses of SFE at dose levels of 1.76, 17.6, and 88 μg/kg for 3 consecutive days. The no observable adverse effect level (NOAEL) and the maximum tolerated dose (MTD) were considered to be greater than 88 μg/kg per day. In studies in beagle dogs, a single i.v. dose of 52.85 μg/kg induced clear clinical signs of toxicity. No adverse cardiovascular effects were observed after individual i.v. injections of 2.64, 10.57, and 52.85 μg/kg. The NOAEL was ≈10.6 μg/kg, and the MTD was ≈53 μg/kg.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B18F%5DSFE%20OR%20%5B18F%5D-2%20OR%20%5B18F%5DWLS1.002%20OR%20%28sigma%201%20receptor%20radioligand%29%29%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B18F%5DSFE%20OR%20%5B18F%5D-2%20OR%20%5B18F%5DWLS1.002%20OR%20%28sigma%201%20receptor%20radioligand%29%29%20AND%20human)]

No publication is currently available.

## NIH Support

NIH NIMH N01MH32001, NIH 1RO1 NS40402, 1RO1 NS40402-03.

## References

1 Waterhouse R.N., Chang R.C., Zhao J., Carambot P.E. (2006). In vivo evaluation in rats of [(18)F]1-(2-fluoroethyl)-4-[(4-cyanophenoxy)methyl]piperidine as a potential radiotracer for PET assessment of CNS sigma-1 receptors. Nucl Med Biol.
2 Waterhouse R.N., Zhao J., Stabin M.G., Ng H., Schindler-Horvat J., Chang R.C., Mirsalis J.C. (2006). Preclinical acute toxicity studies and dosimetry estimates of the novel sigma-1 receptor radiotracer, [18F]SFE. Mol Imaging Biol.
3 Zhao J., Chang R., Carambot P., Waterhouse R.N. (2005). Radiosynthesis and in vivo study of [18F]1-(2-fluoroethyl)-4-[(cyanophenoxy)methyl]piperidine: a promising new sigma-1 receptor ligand. Journal of Labelled Compounds and Radiopharmaceuticals.
4 Lever J.R., Gustafson J.L., Xu R., Allmon R.L., Lever S.Z. (2006). Sigma1 and sigma2 receptor binding affinity and selectivity of SA4503 and fluoroethyl SA4503. Synapse.
5 Skuza G., Wedzony K. (2004). Behavioral pharmacology of sigma-ligands. Pharmacopsychiatry.
6 Skuza G. (2003). Potential antidepressant activity of sigma ligands. Pol J Pharmacol.
7 Ishiguro H., Ohtsuki T., Toru M., Itokawa M., Aoki J., Shibuya H., Kurumaji A., Okubo Y., Iwawaki A., Ota K., Shimizu H., Hamaguchi H., Arinami T. (1998). Association between polymorphisms in the type 1 sigma receptor gene and schizophrenia. Neurosci Lett.
8 Vilner B.J., John C.S., Bowen W.D. (1995). Sigma-1 and sigma-2 receptors are expressed in a wide variety of human and rodent tumor cell lines. Cancer Res.
9 Mach R.H., Gage H.D., Buchheimer N., Huang Y., Kuhner R., Wu L., Morton T.E., Ehrenkaufer R.L. (2005). N-[18F]4'-fluorobenzylpiperidin-4yl-(2-fluorophenyl) acetamide ([18F]FBFPA): a potential fluorine-18 labeled PET radiotracer for imaging sigma-1 receptors in the CNS. Synapse.
10 Hanner M., Moebius F.F., Flandorfer A., Knaus H.G., Striessnig J., Kempner E., Glossmann H. (1996). Purification, molecular cloning, and expression of the mammalian sigma1-binding site. Proc Natl Acad Sci U S A.
11. Mahmood, A. and A.G. Jones, Techneitum Radiopharmaceuticals, in Handbooks of Radiopharmaceuticals, M.J. Welch and C.S. Redvanley, Editors. 2003, John Wiley & Sons, Ltd.: West Sussex. p. 323-349.
12 Waterhouse R.N., Mardon K., Giles K.M., Collier T.L., O'Brien J.C. (1997). Halogenated 4-(phenoxymethyl)piperidines as potential radiolabeled probes for sigma-1 receptors: in vivo evaluation of [123I]-1-(iodopropen-2-yl)-4-[(4-cyanophenoxy)methyl]pip eri dine. J Med Chem.
13 Waterhouse R.N., Collier T.L. (1997). In vivo evaluation of [18F]1-(3-fluoropropyl)-4-(4-cyanophenoxymethyl)piperidine: a selective sigma-1 receptor radioligand for PET. Nucl Med Biol.